# ^111^In-Labeled recombinant gelonin toxin-B lymphocyte stimulator protein fusion protein

Chemical name: | ^111^In-Labeled recombinant gelonin toxin-B lymphocyte stimulator protein fusion protein
Abbreviated name: | [^111^In]-DTPA-rGel/BLyS
Synonym: | TNFSF13b; BAFF; TALL-1; zTNF-4; THANK (for BLyS, from Treml et al. (1))
Agent Category: | Fusion protein
Target: | BLyS receptor 3 (primary target); transmembrane activator, calcium-modulating cyclophilin ligand interactant, and B-cell maturation antigen receptor (secondary targets)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=BLyS&cmd=DetailsSearch)]

The B lymphocyte stimulator (BLyS; for other synonyms see Summary Table above) is a glycoprotein belonging to the tumor necrosis factor cytokine family and promotes the survival, proliferation, and differentiation of the B cells (2). Three different receptors on the B cells (for details, see Wen et al. (2)) are known to bind BLyS; among these, the B cell–activating factor receptor shows the strongest affinity for this cytokine. Although BLyS is overexpressed on B cells of individuals suffering from autoimmune diseases such as lupus, rheumatoid arthritis, etc., the BLyS receptors are known to be expressed on the membrane surface of several types of cancerous tumor cells [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=B%20cell%20cancers)]. Because of its specificity of binding to B cells, BLyS-derived fusion toxins such as the gelonin (Gel)-BLyS fusion protein has been studied by investigators to selectively target and treat B cell malignancies (3-6).

Gel is an N-glycosidase type I ribosome-inactivating plant toxin that lacks a cell binding or a cell internalization domain and is almost non-toxic to intact cells (2, 7). However, mammalian cells can internalize the toxin in association with a carrier, at which point Gel is lethal to the cells because it inhibits protein synthesis completely within 3–4 days of internalization and release within the cell. Recently a recombinant Gel (rGel)-BLyS fusion protein (rGel/BLyS) was constructed by linking rGel to the N-terminus of BLyS, and rGel/BLys was labeled with ^111^In using diethylenetriamine pentaacetic acid (DTPA) to produce the radionuclide chelator [^111^In]-DTPA-rGel/BLyS (2). The biodistribution and tumor-imaging characteristics of [^111^In]-DTPA-rGel/BLyS were then studied in severe combined immunodeficient (SCID) mice bearing B cell lymphoma tumors (2).

### Other Sources of Information

Protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/NM_012452.2) sequences of human BLyS (tumor necrosis factor receptor superfamily, member 13B (TNFRSF13B).

BLyS in OMIM (http://www.ncbi.nlm.nih.gov/omim/603969) (Online Mendelian Inheritance in Man Database).

Clinical trials (http://clinicaltrials.gov/ct2/results?term=BLyS) involving BLyS.

Clinical trials with Belimumab (http://clinicaltrials.gov/ct2/results?term=Belimumab) (anti-BLyS monoclonal antibody).

Protein (http://www.ncbi.nlm.nih.gov/nuccore/DI004841.1) and linear DNA (http://www.ncbi.nlm.nih.gov/nuccore/I41255.1) (source: Patent US 5624827) sequence of plant toxin gelonin (from Gelonium multiflorum).

Gelonin toxin in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=gelonin%20toxin).

What is lupus? Information on MedlinePlus (http://www.nlm.nih.gov/medlineplus/ency/article/000435.htm).

Drugs to treat lupus (http://google2.fda.gov/search?q=Drugs+to+treat+lupus&client=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=8&sort=date%3AD%3AL%3Ad1&entqr=3&oe=UTF-8&ie=UTF-8&ud=1&site=FDAgov&btnG=Search) - FDA site.

Lupus (http://www.genome.gov/gwastudies/index.cfm?pageid=26525384#searchForm) in Genome-Wide Association Studies Database.

What is rheumatoid arthritis? Information on Medline Plus (http://www.nlm.nih.gov/medlineplus/rheumatoidarthritis.html).

Drugs to treat rheumatoid arthritis (http://google2.fda.gov/search?q=Drugs+to+treat+Rheumatoid+arthritis&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=8) - FDA site.

Rheumatoid arthritis (http://www.genome.gov/gwastudies/index.cfm?pageid=26525384#searchForm) in Genome-Wide Association Studies Database.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=rGel/BLyS%20fusion%20protein%20synthesis&cmd=DetailsSearch)]

The rGel/BLyS fusion protein was expressed in and purified from Escherichia coli as described elsewhere (3). The fusion protein was conjugated to DTPA and labeled with ^111^In as detailed by Wen et al. (2). The radiochemical yield of [^111^In]-DTPA-rGel/BLyS was not reported. Radiochemical purity of the final product was >95% as determined with instant thin-layer chromatography (Rf values were not reported). The specific activity of [^111^In]-DTPA-rGel/BLyS was up to 0.3 MBq/μg (8.1 μCi/μg).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=rGel/BLyS%20fusion%20protein%20in%20vitro%20studies&cmd=DetailsSearch)]

The in vitro biological activity of rGel/BLyS and the DTPA-rGel/BLyS conjugate was investigated using JeKo-1 cells (a mantle cell lymphoma cell line) and OCI-Ly10 cells (a diffuse large B cell lymphoma cell line) (2). Both constructs showed a similar cytotoxic effect on the two cell lines, indicating that the conjugation of DTPA to rGel/BLyS did not affect the biological activity of the conjugated fusion protein.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=rGel/BLyS%20fusion%20protein%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-DTPA-rGel/BLyS was studied in SCID mice bearing OCI-Ly10 tumors (2). Five mice received an intravenous injection of the radiochemical (1.85 MBq/6 μg (50 μCi/6 μg)), and 48 h post-injection (p.i.) the animals were euthanized to retrieve the major organs. The amount of radioactivity in each organ was determined and presented as percent injected dose per gram tissue (% ID/g). Maximum label accumulation was detected in the spleen (16.2 ± 3.3% ID/g), followed by the liver (5.4 ± 1.0% ID/g), kidneys (4.0 ± 0.3% ID/g), and bone (1.31 ± 0.4% ID/g). The tumor retained 1.25 ± 0.4% ID/g of the label at 48 h p.i., and the tumor/blood and tumor/muscle ratios were 13.2 and 4.9, respectively.

Micro-SPECT/CT images were acquired from two SCID mice bearing OCI-Ly10 tumors at various predetermined time points for up to 72 h after intravenous injection of [^111^In]-DTPA-rGel/BLyS (2). From the micro-SPECT/CT images, it was evident that, in addition to the tumor, the radioactivity was present in the liver, kidneys, and bone as observed during the biodistribution study. The tumor was clearly visible at 24 h p.i., and the amount of radioactivity in the lesion was reported to peak at this time point followed by a gradual decrease up to 72 h p.i.

From these studies, the investigators concluded that [^111^In]-DTPA-rGel/BLyS can be used to detect B-cell tumors in rodents (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5DDTPA-rGel/BLyS%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5DDTPA-rGel/BLyS%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B111In%5DDTPA-rGel/BLyS%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Treml J.F., Hao Y., Stadanlick J.E., Cancro M.P. (2009). The BLyS family: toward a molecular understanding of B cell homeostasis. Cell Biochem Biophys.
2 Wen, X., M.A. Lyu, R. Zhang, W. Lu, Q. Huang, D. Liang, M.G. Rosenblum, and C. Li, Biodistribution, Pharmacokinetics, and Nuclear Imaging Studies of (111)In-labeled rGel/BLyS Fusion Toxin in SCID Mice Bearing B Cell Lymphoma. Mol Imaging Biol, 2010
3 Lyu M.A., Cheung L.H., Hittelman W.N., Marks J.W., Aguiar R.C., Rosenblum M.G. (2007). The rGel/BLyS fusion toxin specifically targets malignant B cells expressing the BLyS receptors BAFF-R, TACI, and BCMA. Mol Cancer Ther.
4 Lyu M.A., Rai D., Ahn K.S., Sung B., Cheung L.H., Marks J.W., Aggarwal B.B., Aguiar R.C., Gandhi V., Rosenblum M.G. (2010). The rGel/BLyS fusion toxin inhibits diffuse large B-cell lymphoma growth in vitro and in vivo. Neoplasia.
5 Lyu M.A., Sung B., Cheung L.H., Marks J.W., Aggarwal B.B., Aguiar R.C., Rosenblum M.G. (2010). The rGel/BLyS fusion toxin inhibits STAT3 signaling via down-regulation of interleukin-6 receptor in diffuse large B-cell lymphoma. Biochem Pharmacol.
6 Yuan X., Lin X., Manorek G., Howell S.B. (2011). Challenges associated with the targeted delivery of gelonin to claudin-expressing cancer cells with the use of activatable cell penetrating peptides to enhance potency. BMC Cancer.
7 Pirie C.M., Hackel B.J., Rosenblum M.G., Wittrup K.D. (2011). Convergent Potency of Internalized Gelonin Immunotoxins across Varied Cell Lines, Antigens, and Targeting Moieties. J Biol Chem.